# 4-Bromo-1-(3-[^18^F]fluoropropyl)-2-nitroimidazole

Chemical name: | 4-bromo-1-(3-[^18^F]fluoropropyl)-2-nitroimidazole
Abbreviated name: | 4-Br[^18^F]FPN; 4-BrFPN
Synonym:
Agent Category: | Compound
Target: | Hypoxic cells (brain)
Target Category: | Intracellular reduction and binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20FPN%5BAll%20Fields%5D)]

Hypoxia in malignant tumors is thought to be a major factor limiting the efficacy of chemotherapy and radiotherapy, and its accurate diagnosis is considered a very important and urgent problem to address. This has led to the search and development of hypoxia-targeted imaging techniques and non-invasive markers of tumor hypoxia. Among those, ^18^F-labeled nitroimidazoles, used in conjunction with positron emission tomography (PET), offer an alternative that is less invasive and less prone to sampling error than the Eppendorf (oxygen) electrode method (1, 2).

Initial development of nitroimidazoles for in vivo imaging used radiohalogenated derivatives of misonidazole such as fluoromisonidazole ([^18^F]FMISO), which was introduced in 1984 and has now become the most widely used nitroimidazole derivative used with PET. Novel 2-nitroimidazoles, such as [^18^F]FETA (3), [^18^F]FETNIM (4), [^18^F]FPN (5), and 4-Br[^18^F]FPN (6), are also currently under investigation as PET markers for hypoxia.

4-Br[^18^F]FPN was designed to improve the electron affinity of the 2-nitroimidazole ring, when compared with [^18^F]FPN. Indeed, on the basis of molecular orbital calculations, the introduction of a bromine atom at the 4-position in the nitro-bearing ring seems to significantly lower the orbital energy of the lowest unoccupied molecular orbital (E_LUMO_), which may facilitate metabolic reduction and trapping under hypoxia. Studies of 4-Br[^18^F]FPN in rats and mice show enhanced tumor-to-blood and tumor-to-muscle ratios compared with [^18^F]FPN (see details in the Rodents section), but both 4-Br[^18^F]FPN and [^18^F]FPN show a tumor localization less favorable than [^18^F]FMISO.

The oxygen-dependent metabolism of nitroimidazoles is an intracellular process consisting of a series of one-electron reductions. The nitro-radical anion produced in the first reduction step is very reactive toward oxygen, leaving no substrate for the second step of the reduction process. In contrast, an environment of low oxygen concentration induces further reductive reactions that ultimately lead to the formation of either reactive products that are able to covalently bind to cell components or charged species that diffuse slowly out of the tissues (7). The reactive products observed during this multi-step process include nitroso (2e-), hydroxylamine (4e-), and amine (6e-) derivatives. When the fragmentation of the imidazole ring occurs, reactive portions of the molecule, such as glyoxal, bind to macromolecular components of cells in tissues and tumors (2).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%5BAll%20Fields%5D%20AND%20FPN%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

4-Br[^18^F]FPN can be synthesized by a [^18^F]fluoride ion displacement reaction of the tosylate precursor, as reported by Yamamoto et al. (6). In this method, the tosylate is prepared by coupling di-tosyl propylate with 2-nitroimidazole in the presence of triethylamine N,N-dimethylformamide (5). The direct bromination of the tosylate with an excess of Br_2_ in dioxane produces 4-bromo tosylate. 4-BrFPN is obtained by fluoride substitution on the tosylate precursor using tetrabutylammonium fluoride (71% yield).

The radiosynthesis protocol described by Yamamoto et al. (6) leads to a radiochemical yield of about 33% and a radiochemical purity >96% for 4-Br[^18^F]FPN. The total reaction time (including purification) is 40 min. The optimal conditions are obtained with a 15-min reaction time at 80°C in acetonitrile.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29FPN%20AND%20in%20vitro)]

In vitro studies using Chinese hamster V79 cells were performed to assess the radiosensitizing effectiveness of 4-Br[^18^F]FPN on hypoxic cells, as published previously (6). Experiments were conducted in Minimal Essential Medium containing 1% dimethylsulfoxide. The sensitizer enhancement ratio (SER) for 4-Br[^18^F]FPN was calculated as the ratio of the radiation dose required to obtain a survival rate of the cells of 50% in the absence of 4-Br[^18^F]FPN to the radiation dose required in the presence of 4-Br[^18^F]FPN (for a similar survival rate). The SER for 4-Br[^18^F]FPN was 1.65 for a 1 mM concentration, which is not significantly different from those obtained for [^18^F]FMISO (1.60) and [^18^F]FPN (1.81) (5).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29FPN%20AND%20%22rodentia%22%5BMeSH%20Terms%5D)]

The biodistribution of 4-Br[^18^F]FPN was assessed in vivo using normal Wistar rats and C3H mice bearing methylcholanthrene-induced fibrosarcoma tumors at 5, 15, 30, and 60 min after intravenous injection (6).

In normal rats, a fast transport of the radiotracer to tissues was observed, and the extent of defluorination for 4-Br[^18^F]FPN (measured by bone radioactivity) was low during the first 30 min (and increased slightly thereafter). The highest uptakes were in the liver and kidney (13.43 ± 1.73% and 8.00 ± 0.94% dose/g, respectively, at 30 min after injection). The tumor-to-blood ratio at 30 min after injection was 0.777 ± 0.053% dose/g. Brain uptake was rapid, and its maximum (0.41 ± 0.15% dose/g) occurred at <5 min after injection. A rapid washout from the normal brain, with no observed accumulation, was also observed, making 4-Br[^18^F]FPN a potential candidate for PET imaging of brain hypoxic tissue.

In the studies of mice, the tumors did not seem to significantly influence the uptake of 4-Br[^18^F]FPN in normal tissues, and tumors showed a significant retention of the tracer. The concentrations of radioactivity in the tumor mass obtained at 30 and 60 min were 2.4% and 2.1% dose/g, respectively. Those values were found to be higher than those reported for [^18^F]FPN at 30 and 60 min after injection (1.5% and 1.6% dose/g, respectively) using the same rodent tumor model (5). Tumor-to-blood and tumor-to-muscle ratios were 1.19 and 2.05 at 60 min after injection (compared with 0.79 and 1.38 for [^18^F]FPN (5)). A radio-TLC analysis of accumulated radioactivity in tumor and muscle at 60 min after injection showed the formation of polar metabolites, which may indicate the presence of bioreductive metabolism and binding within the tumor.

In summary, the research literature indicates that 4-Br[^18^F]FPN offers more favorable tumor-to-blood and tumor-to-blood ratios, compared with the non-bromide analogs of [^18^F]FPN. Nevertheless, 4-Br[^18^F]FPN has a lower tumor localization than [^18^F]FMISO, although their tumor-to-background ratios do not differ substantially at 30-60 min after injection (6). Therefore, lowering the E_LUMO_ of a molecule appears to be insufficient to improve the biodistribution properties and/or to enhance hypoxic selectivity.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29FPN%20AND%20%28dog%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29FPN%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2818F%29FPN%20AND%20human)]

No publication is currently available.

## References

1 Nunn A, Linder K, Strauss HW. (1995). Nitroimidazoles and imaging hypoxia. Eur J Nucl Med.
2 Hodgkiss RJ. (1998). Use of 2-nitroimidazoles as bioreductive markers for tumour hypoxia. Anticancer Drug Des.
3 Rasey JS, Hofstrand PD, Chin LK, Tewson TJ. (1999). Characterization of [18F]fluoroetanidazole, a new radiopharmaceutical for detecting tumor hypoxia. J Nucl Med.
4 Yang DJ, Wallace S, Cherif A, Li C, Gretzer MB, Kim EE, Podoloff DA. (1995). Development of F-18-labeled fluoroerythronitroimidazole as a PET agent for imaging tumor hypoxia. Radiology.
5 Yamamoto F, Oka H, Antoku S, Ichiya Y, Masuda K, Maeda M. (1999). Synthesis and characterization of lipophilic 1-[18F]fluoroalkyl-2-nitroimidazoles for imaging hypoxia. Biol Pharm Bull.
6 Yamamoto F, Aoki M, Furusawa Y, Ando K, Kuwabara Y, Masuda K, Sasaki S, Maeda M. (2002). Synthesis and evaluation of 4-bromo-1-(3-[18F]fluoropropyl)-2-nitroimidazole with a low energy LUMO orbital designed as brain hypoxia-targeting imaging agent. Biol Pharm Bull.
7 Bruehlmeier M, Roelcke U, Schubiger PA, Ametamey SM. (2004). Assessment of hypoxia and perfusion in human brain tumors using PET with 18F-fluoromisonidazole and 15O-H2O. J Nucl Med.